# ^99m^Tc-Diamine dioxime-Lys-Cys-Arg-Gly-Asp-Cyc-Phe-Cys-polyethylene glycol

Chemical name: | ^99m^Tc-Diamine dioxime-Lys-Cys-Arg-Gly-Asp-Cyc-Phe-Cys-polyethylene glycol
Abbreviated name: | ^99m^Tc-NC100692
Synonym:
Agent category: | Peptide
Target: | Integrin α_v_β_3_
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT)
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=23831237), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=56237028) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=3678&ordinalpos=5&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about Integrin α_v_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NC100692)]

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (1). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). Expression of the α_v_β_3_ integrin is on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues (6, 8, 9). The peptide sequence Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various radiolabeled antagonists have been introduced for imaging of tumors and tumor angiogenesis (10).

Most cyclic RGD peptides are composed of five amino acids. Various cyclic RGD peptides exhibit selective inhibition of binding to α_v_β_3_ integrin (50% inhibition concentration (IC_50_), 7–40 nM) but no inhibition of binding to α_v_β_5_ (IC_50_, 600–4,000 nM) or α_IIb_β_3_ (IC_50_, 700–5,000 nM) integrins (11). Various radiolabeled cyclic RGD peptides and peptidominetics have been found to have high accumulation in tumors in mice (12, 13). Of these developments, [^18^F]galacto-c(RGDfK) has been evaluated in a number of clinical studies for imaging of α_v_β_3_ integrin in cancer patients (14-19). Both α_v_β_3_ and α_v_β_5_ integrins bind to vitronectin (20). However, while the α_v_β_3_ integrin is required for basic fibroblast growth factor–mediated angiogenesis, the α_v_β_5_ integrin is required for vascular endothelial growth factor–induced angiogenesis (21, 22). The peptide Lys-Cys-Arg-Gly-Asp-Cyc-Phe-Cys (NC100717) was identified with phage display screening to be a potent and selective binder to both α_v_β_3_ and α_v_β_5_ integrins (23). A new peptide, NC100692, was derived from NC100717 with addition of diamine dioxime to the ε-amine of Lys and the N-terminal end modified with a short polyethylene glycol unit. Hua et al. (24) reported the development of ^99m^Tc-NC100692 for single-photon emission computed tomography (SPECT) imaging of α_v_β_3_ and α_v_β_5_ integrins in mice with hindlimb ischemia. Bach-Gansmo et al. (25) has performed a preliminary study in patients with breast cancer.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=RGD+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (Integrin α_v_ (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=3678&ordinalpos=5&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=omim&Cmd=DetailsSearch&Term=Integrin%5BAll+Fields%5D+AND+alpha-v%5BAll+Fields%5D)
- Clinical trials (^99m^Tc-NC100692 (http://www.clinicaltrials.gov/ct2/results?term=NC-100692), RGD (http://www.clinicaltrials.gov/ct2/results?term=RGD))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NC100692+synthesis)]

NC100692 was prepared with solid-phase Fmoc chemistry. Edwards et al. (26) prepared ^99m^Tc-NC100692 using labeling kits containing 44 nmol NC100692. ^99m^Tc-Pertechnetate was added for in vivo (2.1 GBq (56 mCi)) and in vitro (100 GBq (2.7 Ci)) binding studies. The radiochemical purity was >90% within 1 h of reconstitution. The specific activities were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NC100692+in+vitro)]

Indrevoll et al. (23) performed in vitro binding assays of ^125^I-echistatin with EA-Hy926 cell membranes containing α_v_β_3_ and α_v_β_5_ integrins. NC100717 and NC100692 had K_i_ (inhibition constant) values of 1.6 ± 1.6 and 3.1 ± 1.6 nM, respectively. Edwards et al. (26) showed that K_d_ (binding constant) values of ^99m^Tc-NC100692 for α_v_β_3_ and α_v_β_5_ integrins were 0.5 ± 0.01 and 0.1 ± 0.04 nM, respectively. No specific binding was observed for α_1_β_1_, α_3_β_1_, α_v_β_1_, and α_IIb_β_5_ integrins.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NC100692+rodentia)]

Hua et al. (24) performed pinhole planar imaging studies of ^99m^Tc-NC100692 in mice with hindlimb ischemia (n = 5–9/group) as an established model of angiogenesis. Mice with femoral occlusion were injected with 55.5 MBq (1.5 mCi) ^99m^Tc-NC100692 on days 1, 3, 7, and 14 of ischemia. Static images were obtained 75 min after ^99m^Tc-NC100692 injection. A significant increase (P < 0.05) in the ischemia/non-ischemia ratio was observed on days 3 (1.5 ± 0.7) and 7 (1.6 ± 0.8) versus the control group (0.9 ± 0.1). ^99m^Tc-NC100692 was cleared quickly from the blood through the kidneys. Ex vivo analysis of excised tissues showed that these ratios were similar to those observed with the in vivo imaging. Immunohistochemistry showed a significant increase (P < 0.05) in RGD staining with endothelial cells within the ischemic hindlimb as compared with the contralateral control hindlimb at days 3, 7, and 14. No blocking experiment was performed.

Edwards et al. (26) performed ex vivo biodistribution studies of ^99m^Tc-NC100692 with normal rats (n = 3/group) at 2, 20, 60, and 240 min after injection. Radioactivity was quickly excreted into urine with little accumulation in other tissues except for the liver and kidneys. The accumulation in the liver and kidneys was reduced with coinjection of NC100692 with the tracer. There was little systemic metabolism of ^99m^Tc-NC100692 up to 20 min after injection. Blood clearance of ^99m^Tc-NC100692 was rapid, and the intact molecule was not detectable at 60 min after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NC100692+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NC100692+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NC100692+human)]

Bach-Gansmo et al. (25) studied 16 breast cancer patients with suggestive mammographic findings and 4 breast cancer patients with benign lesions as determined with ^99m^Tc-NC100692 scintigraphy. All patients received ~700 MBq (19 mCi) ^99m^Tc-NC100692, with 5 patients experiencing non-serious adverse events. Nineteen of 22 (86%) malignant lesions >7 mm in diameter were detected. In another study, Bach-Gansmo et al. (27) performed scintimammography with ^99m^Tc-NC100692 and a dedicated γ-camera, which revealed 9 of 11 lesions (6–20 mm in diameter) in 8 patients with a high suspicion of breast cancer.

## References

1 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
4 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
5 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
6 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
7 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
11 Haubner R., Wester H.J., Burkhart F., Senekowitsch-Schmidtke R., Weber W., Goodman S.L., Kessler H., Schwaiger M. (2001). Glycosylated RGD-containing peptides: tracer for tumor targeting and angiogenesis imaging with improved biokinetics. J Nucl Med.
12 Haubner R., Decristoforo C. (2009). Radiolabelled RGD peptides and peptidomimetics for tumour targeting. Front Biosci.
13 Schottelius M., Laufer B., Kessler H., Wester H.J. (2009). Ligands for mapping alphavbeta3-integrin expression in vivo. Acc Chem Res.
14 Beer A.J., Grosu A.L., Carlsen J., Kolk A., Sarbia M., Stangier I., Watzlowik P., Wester H.J., Haubner R., Schwaiger M. (2007). [18F]galacto-RGD positron emission tomography for imaging of alphavbeta3 expression on the neovasculature in patients with squamous cell carcinoma of the head and neck. Clin Cancer Res.
15 Beer A.J., Haubner R., Goebel M., Luderschmidt S., Spilker M.E., Wester H.J., Weber W.A., Schwaiger M. (2005). Biodistribution and pharmacokinetics of the alphavbeta3-selective tracer 18F-galacto-RGD in cancer patients. J Nucl Med.
16 Beer A.J., Haubner R., Sarbia M., Goebel M., Luderschmidt S., Grosu A.L., Schnell O., Niemeyer M., Kessler H., Wester H.J., Weber W.A., Schwaiger M. (2006). Positron emission tomography using [18F]Galacto-RGD identifies the level of integrin alpha(v)beta3 expression in man. Clin Cancer Res.
17 Beer A.J., Lorenzen S., Metz S., Herrmann K., Watzlowik P., Wester H.J., Peschel C., Lordick F., Schwaiger M. (2008). Comparison of integrin alphaVbeta3 expression and glucose metabolism in primary and metastatic lesions in cancer patients: a PET study using 18F-galacto-RGD and 18F-FDG. J Nucl Med.
18 Beer A.J., Niemeyer M., Carlsen J., Sarbia M., Nahrig J., Watzlowik P., Wester H.J., Harbeck N., Schwaiger M. (2008). Patterns of alphavbeta3 expression in primary and metastatic human breast cancer as shown by 18F-Galacto-RGD PET. J Nucl Med.
19 Haubner R., Weber W.A., Beer A.J., Vabuliene E., Reim D., Sarbia M., Becker K.F., Goebel M., Hein R., Wester H.J., Kessler H., Schwaiger M. (2005). Noninvasive visualization of the activated alphavbeta3 integrin in cancer patients by positron emission tomography and [18F]Galacto-RGD. PLoS Med.
20 Silva R., D'Amico G., Hodivala-Dilke K.M., Reynolds L.E. (2008). Integrins: the keys to unlocking angiogenesis. Arterioscler Thromb Vasc Biol.
21 Friedlander M., Brooks P.C., Shaffer R.W., Kincaid C.M., Varner J.A., Cheresh D.A. (1995). Definition of two angiogenic pathways by distinct alpha v integrins. Science.
22 Hood J.D., Cheresh D.A. (2002). Targeted delivery of mutant Raf kinase to neovessels causes tumor regression. Cold Spring Harb Symp Quant Biol.
23 Indrevoll B., Kindberg G.M., Solbakken M., Bjurgert E., Johansen J.H., Karlsen H., Mendizabal M., Cuthbertson A. (2006). NC-100717: a versatile RGD peptide scaffold for angiogenesis imaging. Bioorg Med Chem Lett.
24 Hua J., Dobrucki L.W., Sadeghi M.M., Zhang J., Bourke B.N., Cavaliere P., Song J., Chow C., Jahanshad N., van Royen N., Buschmann I., Madri J.A., Mendizabal M., Sinusas A.J. (2005). Noninvasive imaging of angiogenesis with a 99mTc-labeled peptide targeted at alphavbeta3 integrin after murine hindlimb ischemia. Circulation.
25 Bach-Gansmo T., Danielsson R., Saracco A., Wilczek B., Bogsrud T.V., Fangberget A., Tangerud A., Tobin D. (2006). Integrin receptor imaging of breast cancer: a proof-of-concept study to evaluate 99mTc-NC100692. J Nucl Med.
26 Edwards D., Jones P., Haramis H., Battle M., Lear R., Barnett D.J., Edwards C., Crawford H., Black A., Godden V. (2008). 99mTc-NC100692--a tracer for imaging vitronectin receptors associated with angiogenesis: a preclinical investigation. Nucl Med Biol.
27 Bach-Gansmo T., Bogsrud T.V., Skretting A. (2008). Integrin scintimammography using a dedicated breast imaging, solid-state gamma-camera and (99m)Tc-labelled NC100692. Clin Physiol Funct Imaging.